# Meta-[radioiodinated]iodobenzylguanidine

Chemical name: | Meta-[radioiodinated]iodobenzylguanidine
Abbreviated name: | [^123^I/^125^I/^131^I]MIBG
Synonym: | m-[^123^I/^125^I/^131^I]MIBG; 2-[(3-iodophenyl)methyl]guanidine; Ultratrace™iobenguane ^131^I; MyoMIBG-^123^I injection; Pheo^®^MIBG-^131^I injection
Agent Category: | Compound
Target: | Norepinephrine receptor
Target Category: | Receptor binding
Method of detection: | SPECT and planer gamma imaging
Source of signal: | ^123^I/^125^I/^131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG)]

Meta-iodobenzylguanidine (MIBG) is a norepinephrine (NE) analog that contains a benzyl and a guanidine group. Because it structurally resembles NE, neuroendocrine cells take up MIBG through an active mechanism and store it in the neurosecretory granules. This leads to specific concentration of the molecule in the neuroendocrine cells. MIBG radiolabeled with iodine (as ^123^I, ^125^I, or ^131^I) is used for scintigraphy or therapy of a variety of tumors that have an endocrine origin (1, 2). In addition, ^123^I-labeled MIBG ([^123^I]MIBG) is used for sympathetic innervation scintigraphy of the heart (3), and [^125^I]MIBG is used to study adrenergic nerve changes during physiological stress, disease, or after the treatment of heart function (4). Among the iodine radiolabeled homologs of MIBG, [^123^I]MIBG and [^131^I]MIBG are used most often for diagnosis. In general, [^123^I]MIBG is the clinical agent of choice because of its low effective dose and high-quality single-photon emission computed tomography (SPECT) results for cardiac sympathetic nerves, pheochromocytomas, and neuroendocrine tumors (2, 5).

Although [^131^I]MIBG is approved by the United States Food and Drug Administration as an investigational new drug for clinical use (6, 7), [^123^I]MIBG is not (2, 5). [^131^I]MIBG is currently undergoing evaluation in phase 1 and phase 1/2 clinical trials (http://www.molecularinsight.com/Azedra patient recruitment brochure NET Flyer 8 29.pdf) in the United States for the treatment of neuroendocrine tumors. [^123^I]MIBG is commercially available in Europe and both [^123^I]MIBG and [^131^I]MIBG are available as diagnostic radiopharmaceuticals in Japan. Guidelines for the use of [^123^I/^131^I]MIBG for tumor imaging are available from the European Association of Nuclear Medicine website.

## Synthesis

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG%20synthesis)

The synthesis of [^123^I/^125^I/^131^I]MIBG was described by Wieland et al. in a US patent (8). The radiolabeled compounds were generated by radioiodide exchange with the appropriate iodine radioisotope using sodium iodide. In this chapter, only the synthesis of [^123^I]MIBG is described. The other two radioisotopes ([^125^I/^131^I]MIBG) were synthesized using the same procedure, which provided a similar radiochemical yield and purity.

To start, m-iodobenzylamine was mixed with cyanamide and stirred with heating at 100ºC for 4 h to obtain a solid that was dissolved in water. To this, a solution of potassium bicarbonate was added dropwise with stirring and the precipitated meta-iodoguanidine bicarbonate was collected. The precipitate was washed with water and dried in vacuo with a yield of 85%. The bicarbonate salt was suspended in water and sulfuric acid was slowly added. The resulting suspension was warmed to a solution and the desired m-iodobenzylguanidine sulfate was crystallized when it cooled to room temperature. The crystals were washed with cold water and dried in vacuo with a yield of 78%. The sulfate was dissolved in water and refluxed at 140ºC in an oil bath with Na[^123^I] for 20–30 min, during which time the water was allowed to evaporate. More water was added while the temperature was maintained, and the water was again allowed to evaporate; this procedure was repeated several times for a total reaction time of 3 h to obtain a residue. The residue was redissolved in water and purified through a glass column packed with Cellex D anion exchange cellulose to remove any unreacted and radiolabeled iodide and iodate.

Purity of the product was determined by thin-layer chromatography to be >98%, and the absence of rearranged isomeric impurities was confirmed with high-performance liquid chromatography on a micro Bondapak C18 column. The radioiodinated product yield was 90–95% with a specific activity of 20.35–410.7 MBq/μmol (0.56–11.10 mCi/μmol) and a purity of >98%.

Methods for the synthesis of no-carrier-added (NCA) [^123^I]MIBG and [^131^I]MIBG are also available (9-11).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG%20in%20vitro)]

The differential toxicity of [^123^I]MIBG in neuroblastoma (NB) cell lines (SK-N-SH and SK-N-BE(2)) and human cells of hematopoietic lineage (HL-60 and bone marrow stem cells) was investigated (12). [^123^I]MIBG strongly inhibited proliferation of the NB cell lines but was sparing for cells of hematopoietic lineage. The investigators also observed that meta-trimethylsilylbenzylguanidine (MTBG), one of the precursors used for the synthesis of NCA MIBG, was toxic towards the NB and Hl-60 cells. This indicated that NCA preparations of MIBG should be further purified before clinical use.

The use of either [^125^I]MIBG or [^131^I]MIBG, alone or in combination, to treat neuroblastoma multicellular tumor spheroids derived from the SK-N-SH cell line was investigated in vitro (13). The investigators concluded that [^125^I]MIBG by itself was not superior to [^131^I]MIBG for treatment; however, a combination of the two radiotracers was a more effective treatment than using [^131^I]MIBG alone.

The uptake of [^125^I]MIBG was determined in a pheochromocytoma cell line (PC-12) after exposure to 1-methyl-4-phenyl-1,2,3,6-terrahydroxypyridine (MPTP), a chemical used to induce Parkinson’s disease in mice (14). The accumulation of [^125^I]MIBG in the PC-12 cells was blocked almost completely by MPTP, which indicated that neurons were damaged by the exposure to MPTP.

The application of gene therapy with [^131^I]MIBG was explored by Fullerton et al. in EJ138 cells, a bladder cancer cell line (15). The cells were transfected with a gene encoding the noradrenaline transporter under the control of tumor-specific promoters. The uptake of [^131^I]MIBG was assessed in these cells. Radiolabel accumulation and cell death were observed to be dose-dependent. The investigators suggested the possible use of this strategy in the treatment of bladder cancer.

Anti-cancer drugs such as topotecan, cisplatin, and doxorubicin were shown to induce increased accumulation of [^131^I]MIBG in NB cells (16, 17).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG%20rodentia)]

The use of NCA and carrier-added [^123^I]MIBG for the assessment of cardiac sympathetic nerve activity in rats was evaluated by SPECT scintigraphy (18). A higher cardiac uptake of the NCA than of the carrier-added radiolabel was observed, and the investigators concluded that the NCA variety could provide a better scintigraphic assessment of the myocardial sympathetic nervous system.

In a study designed to investigate the distribution of [^125^I]MIBG in various organs of the rat, Wieland et al. showed that the radiotracer accumulated mainly in the heart, liver, and lungs of these animals (19). Among these organs, the heart had the highest accumulation of label. Other studies demonstrated that [^125^I]MIBG could be used to investigate the in vivo functioning of rat adrenergic neurons (4) and modulation of the atrioventricular nodal and bundle (His bundle) sympathetic activity in the heart (20). Sisson et al (21). suggested that the movement of [^125^I]MIBG may be used as an indication of neuronal injury and heart function in rats. This radiotracer was also used to demonstrate that the endocardial and epicardial layers of the left ventricle in the rat heart were probably innervated differently (22). Wakasugi et al (23, 24). demonstrated that [^125^I]MIBG could be used to determine adriamycin cardiomyopathy in rats.

In a study with Syrian hamsters, a reduced accumulation of [^125^I]MIBG in the heart during cardiomyopathy was shown to be caused by its release from neuronal junctions as a result of activation of the renin-angiotensin system (25).

Intraperitoneal pretreatment of mice bearing xenografts of human NB cell lines with cisplatin and doxorubicin showed an increased accumulation of [^125^I]MIBG in the tumors (17), which indicated that the drugs selectively increase radiation doses delivered to neuroblastoma tumors.

Mice pretreated with MPTP can be used as an animal model for Parkinson’s disease. Takatsu et al. (26) observed a significantly reduced cardiac accumulation of [^125^I]MIBG in MPTP-treated animals and suggested that this agent or unknown toxic substrates in experimental or human Parkinson’s disease may damage the postganglionic sympathetic nerves.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG%20Non-Primate%20Mammals)]

The ex vivo distribution of [^125^I]MIBG was studied in different organs of the dog (19). Accumulation of the tracer was observed primarily in the heart, liver, and lungs, which is similar to observations in the rat. The dog heart was shown to take up the label rapidly and lose it gradually over 24 h. Pretreatment of dogs with reserpine resulted in a 30% decrease in [^125^I]MIBG accumulation (19). Sisson et al (4). demonstrated that [^125^I]MIBG could be used to measure acute changes in neuronal activity of the dog heart. The distribution of [^125^I]MIBG was investigated in normal and denervated canine hearts (27). Normal hearts showed an uptake of MIBG at 5 min and after 3 hrs, but the denervated hearts showed an uptake only at the early time point. This indicated that the label accumulated mainly in the neuronal tissue and was quickly lost from the non-neuronal tissues.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MIBG%20Non-human%20Primate)]

The distribution of [^125^I]MIBG has been studied in various organs of the monkey (19, 28). In these animals highest uptake was observed in the liver, followed by the heart and lungs. [^125^I]MIBG was also used as a myocardial imaging agent in the monkeys.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=125I%20MIBG%20human)]

Kline et al. (29) demonstrated the use of [^125^I]MIBG as a myocardial imaging agent in humans. The distribution of this tracer was studied in normal and transplanted human hearts (27). The investigators showed significant accumulation of radiolabel at 5 min and 3 hr in the normal heart; however, the transplanted organ showed no localization of the label either at 5 min or 3 hr, indicating that the non-neuronal uptake mechanism for this compound is not significant in humans. Regional sympathetic denervation of the heart was suggested to be the cause of the lack of radioactivity uptake by the transplanted organs. Sisson et al. (30) showed that [^125^I]MIBG could be used to determine the regional distribution and functioning of the human adrenergic nervous system.

The uptake of [^125^I]MIBG in neuroblastoma tumors in children was investigated by Moyes et al. (31). The investigators observed that quantitative uptake of the label varied between patients and even between different parts of the individual tumors. Also, the more differentiated tumors took up higher amounts of label compared to the undifferentiated tumors.

The use of [^131^I]MIGB as an investigational new drug for the treatment of refractory NB and malignant pheochromocytomas (PHEO) or paragangliomas (PGL) is being evaluated (6, 7). The investigators reported that 67% of the patients with malignant PHEO or PGL who showed a good uptake of the radiolabeled compound had either complete remission, partial response, or stable disease (6). Because of its high response rate and low nonhematologic toxicity, the incorporation of [^131^I]MIBG as an agent for a multi-modal therapy of NB was suggested (7).

## References

1 Guller U., Turek J., Eubanks S., Delong E.R., Oertli D., Feldman J.M. (2006). Detecting pheochromocytoma: defining the most sensitive test. Ann Surg.
2 Rufini V., Calcagni M.L., Baum R.P. (2006). Imaging of neuroendocrine tumors. Semin Nucl Med.
3 Camacho V., Carrio I. (2007). Targeting neuronal dysfunction and receptor imaging. Curr Opin Biotechnol.
4 Sisson J.C., Bolgos G., Johnson J. (1991). Measuring acute changes in adrenergic nerve activity of the heart in the living animal. Am Heart J.
5 Eisenhofer G., Pacak K., Goldstein D.S., Chen C., Shulkin B. (2000). 123I-MIBG scintigraphy of catecholamine systems: impediments to applications in clinical medicine. Eur J Nucl Med.
6 Fitzgerald P.A., Goldsby R.E., Huberty J.P., Price D.C., Hawkins R.A., Veatch J.J., Dela Cruz F., Jahan T.M., Linker C.A., Damon L., Matthay K.K. (2006). Malignant pheochromocytomas and paragangliomas: a phase II study of therapy with high-dose 131I-metaiodobenzylguanidine (131I-MIBG). Ann N Y Acad Sci.
7 Matthay K.K., Yanik G., Messina J., Quach A., Huberty J., Cheng S.C., Veatch J., Goldsby R., Brophy P., Kersun L.S., Hawkins R.A., Maris J.M. (2007). Phase II study on the effect of disease sites, age, and prior therapy on response to iodine-131-metaiodobenzylguanidine therapy in refractory neuroblastoma. J Clin Oncol.
8. Weiland, D.M., L.E. Brown, W.H. Beierwaltes, and J.L. Wu, Imaging agent and method of use. United States Patent number 4584187, 1986.
9 Gaze M.N., Mairs R.J., Vaidyanathan G., Zalutsky M.R. (1994). Synthesis of carrier-free 131I-meta-iodobenzyl-guanidine by novel routes to enhance therapeutic efficiency in neuroblastoma. Prog Clin Biol Res.
10 Mairs R.J., Gaze M.N., Watson D.G., Skellern G.G., Constable P., McKellar K., Owens J., Vaidyanathan G., Zalutsky M.R. (1994). Carrier-free 131I-meta-iodobenzylguanidine: comparison of production from meta-diazobenzylguanidine and from meta-trimethylsilylbenzylguanidine. Nucl Med Commun.
11 Samnick S., Bader J.B., Muller M., Chapot C., Richter S., Schaefer A., Sax B., Kirsch C.M. (1999). Improved labelling of no-carrier-added 123I-MIBG and preliminary clinical evaluation in patients with ventricular arrhythmias. Nucl Med Commun.
12 He Y., Das B., Baruchel S., Kumar P., Wiebe L., Reilly R.M. (2004). Meta-[123I]iodobenzylguanidine is selectively radiotoxic to neuroblastoma cells at concentrations that spare cells of haematopoietic lineage. Nucl Med Commun.
13 Weber W., Weber J., Senekowitsch-Schmidtke R. (1996). Therapeutic effect of m-[131I]- and m-[125I]iodobenzylguanidine on neuroblastoma multicellular tumor spheroids of different sizes. Cancer Res.
14 Takatsu H., Wada H., Maekawa N., Takemura M., Saito K., Fujiwara H. (2002). Significant reduction of 125 I-meta-iodobenzylguanidine accumulation directly caused by 1-methyl-4-phenyl-1,2,3,6-tetrahydroxypyridine, a toxic agent for inducing experimental Parkinson's disease. Nucl Med Commun.
15 Fullerton N.E., Mairs R.J., Kirk D., Keith W.N., Carruthers R., McCluskey A.G., Brown M., Wilson L., Boyd M. (2005). Application of targeted radiotherapy/gene therapy to bladder cancer cell lines. Eur Urol.
16 McCluskey A.G., Boyd M., Gaze M.N., Mairs R.J. (2005). [131I]MIBG and topotecan: a rationale for combination therapy for neuroblastoma. Cancer Lett.
17 Meco D., Lasorella A., Riccardi A., Servidei T., Mastrangelo R., Riccardi R. (1999). Influence of cisplatin and doxorubicin on 125I-meta-iodobenzylguanidine uptake in human neuroblastoma cell lines. Eur J Cancer.
18 Verberne H.J., de Bruin K., Habraken J.B., Somsen G.A., Eersels J.L., Moet F., Booij J., van Eck-Smit B.L. (2006). No-carrier-added versus carrier-added123I-metaiodobenzylguanidine for the assessment of cardiac sympathetic nerve activity. Eur J Nucl Med Mol Imaging.
19 Wieland D.M., Brown L.E., Rogers W.L., Worthington K.C., Wu J.L., Clinthorne N.H., Otto C.A., Swanson D.P., Beierwaltes W.H. (1981). Myocardial imaging with a radioiodinated norepinephrine storage analog. J Nucl Med.
20 Lurie K.G., Dae M.W., Dutton J., Velazquez-Rocha S.J., O'Connell J.W. (1995). Metaiodobenzylguanidine as an index of atrioventricular nodal adrenergic activity. J Nucl Med.
21 Sisson J.C., Wieland D.M., Sherman P., Mangner T.J., Tobes M.C., Jacques S. (1987). Metaiodobenzylguanidine as an index of the adrenergic nervous system integrity and function. J Nucl Med.
22 Matsunari I., Bunko H., Taki J., Nakajima K., Muramori A., Kuji I., Miyauchi T., Tonami N., Hisada K. (1993). Regional uptake of iodine-125-metaiodobenzylguanidine in the rat heart. Eur J Nucl Med.
23 Wakasugi S., Fischman A.J., Babich J.W., Aretz H.T., Callahan R.J., Nakaki M., Wilkinson R., Strauss H.W. (1993). Metaiodobenzylguanidine: evaluation of its potential as a tracer for monitoring doxorubicin cardiomyopathy. J Nucl Med.
24 Wakasugi S., Wada A., Hasegawa Y., Nakano S., Shibata N. (1992). Detection of abnormal cardiac adrenergic neuron activity in adriamycin-induced cardiomyopathy with iodine-125-metaiodobenzylguanidine. J Nucl Med.
25 Takatsu H., Uno Y., Fujiwara H. (1995). Modulation of left ventricular iodine-125-MIBG accumulation in cardiomyopathic Syrian hamsters using the renin-angiotensin system. J Nucl Med.
26 Takatsu H., Nishida H., Matsuo H., Watanabe S., Nagashima K., Wada H., Noda T., Nishigaki K., Fujiwara H. (2000). Cardiac sympathetic denervation from the early stage of Parkinson's disease: clinical and experimental studies with radiolabeled MIBG. J Nucl Med.
27 Dae M.W., De Marco T., Botvinick E.H., O'Connell J.W., Hattner R.S., Huberty J.P., Yuen-Green M.S. (1992). Scintigraphic assessment of MIBG uptake in globally denervated human and canine hearts--implications for clinical studies. J Nucl Med.
28 Wieland D.M., Brown L.E., Tobes M.C., Rogers W.L., Marsh D.D., Mangner T.J., Swanson D.P., Beierwaltes W.H. (1981). Imaging the primate adrenal medulla with [123I] and [131I] meta-iodobenzylguanidine: concise communication. J Nucl Med.
29 Kline R.C., Swanson D.P., Wieland D.M., Thrall J.H., Gross M.D., Pitt B., Beierwaltes W.H. (1981). Myocardial imaging in man with I-123 meta-iodobenzylguanidine. J Nucl Med.
30 Sisson J.C., Shapiro B., Meyers L., Mallette S., Mangner T.J., Wieland D.M., Glowniak J.V., Sherman P., Beierwaltes W.H. (1987). Metaiodobenzylguanidine to map scintigraphically the adrenergic nervous system in man. J Nucl Med.
31 Moyes J.S., Babich J.W., Carter R., Meller S.T., Agrawal M., McElwain T.J. (1989). Quantitative study of radioiodinated metaiodobenzylguanidine uptake in children with neuroblastoma: correlation with tumor histopathology. J Nucl Med.